# VCAM-1 internalizing peptide-28 nanoparticles

Chemical name: | VCAM-1 internalizing peptide-28 nanoparticles
Abbreviated name: | VINP-28 NP
Synonym: | VHPKQHRGGSK(FITC)GC-CLIO-Cy5.5 nanoparticles, VINP-28-CLIO-Cy5.5 nanoparticles
Agent Category: | Peptide
Target: | Vascular cell adhesion molecule-1 (VCAM-1)
Target Category: | Receptor binding
Method of detection: | Magnetic resonance imaging (MRI), optical (near-infrared (NIR) fluorescence)
Source of signal/contrast: | Iron oxide, Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=54648638), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=46249772) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412) for more information about VCAM-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=VCAM-1+nanoparticle)]

Optical fluorescence imaging is increasingly being used to obtain images of biological functions of specific targets in vitro and in small animals (1, 2). Near-infrared (NIR) fluorescence (700–900 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in vitro and in small animals.

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used to create images because of their abundance in water molecules, which comprise >80% of most soft tissues. The contrast of proton MRI images depends mainly on the density of nuclei (proton spins), the relaxation times of the nuclear magnetization (T1, longitudinal; T2, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T1 and T2 relaxation times of the surrounding nuclei, mainly the protons of water. T2* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (3). Cross-linked iron oxide (CLIO) nanoparticles and other iron oxide formulations affect T2 primarily and lead to a decreased signal.

A multimodal nanoparticle probe that consists of a contrast agent and a NIR fluorochrome may provide consistent information. CLIO nanoparticles can be internalized by cells of the reticuloendothelial system and have long circulating times within an animal body. The blood half-life of CLIO is ~10 h in mice (4). The accumulation of nanoparticles in cells causes a reduction in signal intensity with T2-weighted (T2*W) spin-echo pulse sequences. NIR fluorochromes (e.g., Cy5.5) provide an improved optical (NIR) signal from tissue. CLIO-Cy5.5 has been developed as a multimodal probe for imaging.

Endothelial cells are important in inflammatory responses (5, 6). Bacterial lipopolysaccharide, virus, inflammation, and tissue injury increase tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and other cytokine and chemokine secretion. Emigration of leukocytes from blood is dependent on their ability to roll along endothelial cell surfaces and subsequently adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell-surface adhesion molecules, such as intracellular adhesion molecule-1 (ICAM-1), vascular cell adhesion molecule-1 (VCAM-1), integrins, and selectins. Chemokines are chemotactic toward leukocytes and toward sites of inflammation and tissue injury. The movement of leukocytes through endothelial junctions into the extravascular space is highly orchestrated through various interactions with different adhesion molecules on endothelial cells (7).

VCAM-1 is found in very low amounts on the cell surface of resting endothelial cells and other vascular cells, such as smooth muscle cells and fibroblasts (8-12). VCAM-1 binds to very late antigen-4 (VLA-4) integrin on the cell surface of leukocytes. IL-1 and TNFα increase expression of VCAM-1 and other cell adhesion molecules on the vascular endothelial cells, which leads to leukocyte adhesion to the activated endothelium. Furthermore, VCAM-1 expression is also induced by oxidized low-density lipoproteins under atherogenic conditions (13). Overexpression of VCAM-1 by atherosclerotic lesions plays an important role in their progression toward vulnerable plaques, which may erode and rupture. CLIO nanoparticle targeted with anti–VCAM-1 antibody is being developed as a non-invasive agent for VCAM-1 expression in vascular endothelial cells during different stages of inflammation in atherosclerosis (14). A linear peptide (VHPKQHR) homologous to VLA-4 bound to and was internalized by cells expressing VCAM-1 (15, 16). VHPKQHRGGSK(FITC)GC (VINP-28) with fluorescein isothiocyanate (FITC) was synthesized and conjugated to CLIO-Cy5.5 nanoparticle to form a multimodal imaging agent (VINP-28-CLIO-Cy5.5) that consists of CLIO nanoparticle with attachment of VINP-28 and Cy5.5.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+nanoparticle+synthesis)]

The synthesis of VINP-28-CLIO-Cy5.5 nanoparticles was described by Kelly et al. (15) and Nahrendorf et al. (16). The amino-CLIO nanoparticles (62 amino groups per nanoparticle, 3 nm Fe core, 38 nm in diameter with dextran coating, R2 = 62 mM^-1^s^-1^) were labeled with Cy5.5 using N-hydroxysuccinimide to form amino-CLIO-Cy5.5 nanoparticles, which were then derivatized with succinimidyl iodoacetate and conjugated with VINP-28 via the cysteine residue in the linker region. The purified VINP-28-CLIO-Cy5.5 nanoparticles had 12 VINP-28 and 2 Cy5.5 molecules per nanoparticle.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+nanoparticle+in+vitro)]

Kelly et al. (15) performed cell-binding assays with VINP-28 using murine cardiac endothelial cells with a binding affinity of 33.7 ± 9 nM as determined with fluorescence flow cytometry. The peptide accumulated intracellularly, and the accumulation was significantly inhibited (P < 0.001) by 75% with soluble VCAM-1 but not with ICAM-1. VINP-28-CLIO-Cy5.5 nanoparticles exhibited a 3.2-fold increased in fluorescent signal over the VINP-28. VINP-28-CLIO-Cy5.5 bound to endothelial cells with 9-fold and 5-fold increase in fluorescent signal over macrophages and fibroblasts, respectively. In vitro MRI studies with VINP-28-CLIO-Cy5.5 nanoparticles in human carotid endarterectomy atheroma specimens showed a T2 reduction of 3.8 ± 1.7 ms (P < 0.05 versus saline), which is consistent with fluorescence imaging and immunohistochemistry and indicates the presence of VCAM-1 expression cells in the atheroma plaque.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+nanoparticle+rodentia)]

Nahrendorf et al. (16) performed intravital confocal microscopy in C57BL/6 mice after subcutaneous injection of TNFα to the right ear, resulting in vascular inflammation in 24 h. After injection of VINP-28-CLIO-Cy5.5, there was a strong enhancement in endothelial cells expressing VCAM-1 in the inflamed ear. In normal mice, VINP-28-CLIO-Cy5.5 exhibited a blood half-life of 17.7 h. The organ with the highest accumulation (injected dose/g) at 6 h after injection was the liver (2.83%), followed by the kidneys (1.87%), heart (0.90%), spleen (0.82%), lungs (0.77%), muscle (0.22%), and fat (0.20%).

Nahrendorf et al. (16) performed in vivo MRI and optical imaging in apolipoprotein E–deficient (apoE^-/-^) mice (n = 28) after injection with VINP-28-CLIO-Cy5.5 or saline. There was a 77% (P < 0.05) decrease in MR signal intensity in the aortic wall 48 h after injection. The aortic arch exhibited a high plaque/background ratio of 9.25 ± 2.5 (>350% higher than saline control), revealing signal enhancement in the aortic arch of mice that received VINP-28-CLIO-Cy5.5 (P < 0.05). VINP-28-CLIO-Cy5.5 fluorescence signal colocalized with endothelial cells and macrophages that expressed VCAM-1 and was spatially distinct compared with untargeted control nanoparticles. Atheromata of atorvastatin-treated apoE^-/-^ mice on a high-cholesterol diet showed reduced VINP-28-CLIO-Cy5.5 deposition and VCAM-1 expression as compared with untreated mice (P < 0.05). No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+nanoparticle+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+nanoparticle+(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+nanoparticle+human)]

No publication is currently available.

## NIH Support

HL078641, HL36436, HL080731, P01-AI054904

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
4 Wunderbaldinger P., Josephson L., Bremer C., Moore A., Weissleder R. (2002). Detection of lymph node metastases by contrast-enhanced MRI in an experimental model. Magn Reson Med.
5 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
6 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
7 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
8 Bochner B.S., Luscinskas F.W., Gimbrone M.A., Newman W., Sterbinsky S.A., Derse-Anthony C.P., Klunk D., Schleimer R.P. (1991). Adhesion of human basophils, eosinophils, and neutrophils to interleukin 1-activated human vascular endothelial cells: contributions of endothelial cell adhesion molecules. J Exp Med.
9 Kume N., Cybulsky M.I., Gimbrone M.A. (1992). Lysophosphatidylcholine, a component of atherogenic lipoproteins, induces mononuclear leukocyte adhesion molecules in cultured human and rabbit arterial endothelial cells. J Clin Invest.
10 Leung K.H. (1999). Release of soluble ICAM-1 from human lung fibroblasts, aortic smooth muscle cells, dermal microvascular endothelial cells, bronchial epithelial cells, and keratinocytes. Biochem Biophys Res Commun.
11 Luscinskas F.W., Cybulsky M.I., Kiely J.M., Peckins C.S., Davis V.M., Gimbrone M.A. (1991). Cytokine-activated human endothelial monolayers support enhanced neutrophil transmigration via a mechanism involving both endothelial-leukocyte adhesion molecule-1 and intercellular adhesion molecule-1. J Immunol.
12 Nagel T., Resnick N., Atkinson W.J., Dewey C.F., Gimbrone M.A. (1994). Shear stress selectively upregulates intercellular adhesion molecule-1 expression in cultured human vascular endothelial cells. J Clin Invest.
13 Aikawa M., Libby P. (2004). The vulnerable atherosclerotic plaque: pathogenesis and therapeutic approach. Cardiovasc Pathol.
14 Tsourkas A., Shinde-Patil V.R., Kelly K.A., Patel P., Wolley A., Allport J.R., Weissleder R. (2005). In vivo imaging of activated endothelium using an anti-VCAM-1 magnetooptical probe. Bioconjug Chem.
15 Kelly K.A., Nahrendorf M., Yu A.M., Reynolds F., Weissleder R. (2006). and In Vivo Phage Display Selection Yields Atherosclerotic Plaque Targeted Peptides for Imaging. Mol Imaging Biol.
16 Nahrendorf M., Jaffer F.A., Kelly K.A., Sosnovik D.E., Aikawa E., Libby P., Weissleder R. (2006). Noninvasive vascular cell adhesion molecule-1 imaging identifies inflammatory activation of cells in atherosclerosis. Circulation.